# Gold nanoparticles coated with dithiolated diethylenetriamine pentaacetic acid-gadolinium chelate

Chemical name: | Gold nanoparticles coated with dithiolated diethylenetriamine pentaacetic acid-gadolinium chelate
Abbreviated name: | Au@DTDTPA-Gd_50_
Synonym: | Au@DTDTPA-Gd
Agent Category: | Nanoparticles
Target: | Non-targeted
Target Category: | Non-targeted
Method of detection: | Multimodality imaging (magnetic resonance imaging/computed tomography (MRI/CT))
Source of signal / contrast: | Au and Gd(III)
Activation: | No
Studies: | - Rodents | No structure is available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=multimodality+imaging+and+review)]

The gold nanoparticles (AuNPs) coated with dithiolated diethylenetriamine pentaacetic acid (DTDTPA)-gadolinium (Gd(III)) chelate, abbreviated as Au@DTDTPA-Gd_50_ (Au = 10 mg/ml; Gd(III) = 5 mM), are a magnetic resonance imaging (MRI)/computed tomography (CT) dual-imaging agent synthesized by Alric et al. for MRI/CT bimodal imaging (1).

Development of hybrid imaging technology has triggered great effort in probe development to boost the benefits of hybrid instrument technology (2-4). In contrast to other agents, multimodal imaging agents for MRI/CT have rarely been explored, although MRI and CT are frequently applied to the same patients for precise diagnosis and treatment evaluation (5-7). Recently, AuNPs have been shown to induce strong contrast enhancement as X-ray contrast agents (1, 8). These particles exhibit a higher X-ray absorption coefficient than iodinated compounds (5.16 and 1.94 cm^2^/g, respectively, at 100 keV). Furthermore, AuNPs are easily controlled with regard to size, shape, and surface modification (9). Gd(III) also possesses a higher X-ray absorption coefficient (3.11 cm^2^/g at 100 keV) than iodine, although this value is lower than that of gold. Interestingly, when Gd(III) ions are bound to NPs, they exhibit a much higher relaxivity than that of clinically approved Gd(III)-chelates (8, 9). Sanchez et al. have shown that the water-soluble apoferritin-encapsulated gadolinium oxide-hydroxide NPs (Gd-Apoferritin) exhibit 10 and 70 times higher T1 and T2 relaxivity values, respectively, than those of classic Gd(III)-complexes (Omniscan^®^ and Gd-DTPA) (8).

On the basis of these facts, Gd(III)-coated AuNPs have been hypothesized to be an efficient dual agent for MRI/CT imaging. Alric et al. demonstrated that Gd(III) chelate-coated AuNPs (Au@DTDTPA-Gd_50_) provide strong X-ray absorption and R1 relaxivity (1). The contrast enhancement in MRI stems from the presence of Gd(III) ions that are entrapped in the organic shell, whereas the gold core provides strong X-ray absorption. These particles are small enough (2–2.5 nm) to circulate freely in the blood vessels without undesirable accumulation in organs such as lungs, spleen, and liver. Park et al. developed a MRI/CT dual-imaging agent with Gd(III) and gold reporters (Au@GdL) (9). Au@GdL NPs are generated by encapsulating gold cores within a multilayered organic shell, and they have been shown to accumulate in tumor xenografts in animals (9). This chapter summarizes the data obtained with Au@DTDTPA-Gd_50_ in MRI/CT imaging (1).

### Related Resource Links:

- Multimodality imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=multimodality%5bAll+Fields%5d+OR+multimodal%5bAll+Fields%5d+AND+micad%5bbook%5d)
- Multimodality imaging clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=multimodality+imaging)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20188545)]

Au@DTDTPA-Gd NPs were synthesized by reducing gold salt (HAuCl_4_ ·3H_2_O) with sodium borohydride (NaBH_4_) in the presence of dithiolated derivatives of diethylenetriamine pentaacetic acid (1). With a molar ratio of 0.104 for gold to NaBH_4_ and 1.020 for gold to DTDTPA, the Au@DTDTPA-Gd NPs were composed of an AuNP core (2.4 nm in diameter) and an organic shell with ~150 DTDTPA and ~150 Gd(III) per particle (Au@DTDTPA_150_). However, the incorporation of 150 Gd(III) per particle altered the colloidal stability for gold content to a great extent (>1 mg/ml). This lack of stability was overcome by reducing Gd(III) to ~50 per particle (Gd to DTDTPA molar ratio: 0.33) (Au@DTDTPA-Gd_50_). The zeta potential of Au@DTDTPA-Gd_50_ was −25 mV at pH 7.4 with 0.01 M NaCl, which is weaker than that of Au@DTDTPA (−32 mV), but the negative charge was sufficiently strong to ensure the colloidal stability (gold content: 10 mg/ml) in the physiological medium (pH 7.4, 150 mM NaCl) for at least 1 week.

Synchrotron radiation computed tomography (SRCT) of the phantoms containing Au@DTDTPA at various gold concentrations (0.14–10 mg/ml; 0.71 ≤ Au ≤ 50.7 mM) and Au@DTDTPA-Gd_50_ (5.6 mg/ml; Au = 28.4 mM) showed that these particles induced a contrast enhancement when the gold concentration was at least equal to 1.4 mg/ml. Conventional CT analysis revealed that 50.7 mM Au@DTDTPA (10 mg Au/ml) exhibited an equivalent X-ray absorption of 280 mM iodine (35 mg iodine/ml). The R1 relaxivity of the Au@DTDTPA-Gd_50_ was similar to that of Au@DTDTPA_150_ (3.9 mM^-1^s^-1^) (1). Au@DTDTPA-Gd_50_ (10 mg Au/ml and 5 mM Gd(III) in 150 mM NaCI hepes-buffered solution at pH 7.4) was used for in vivo studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20188545)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/20188545)]

SRCT and MRI were performed before and after intravenous injection of 300 µl Au@DTDTPA-Gd_50_ colloid in mice and 0.6–1.8 ml Au@DTDTPA-Gd_50_ colloid in rats (1).

For SRCT, kidneys could be detected at 3 min after injection, and the ureter and urinary tract could be delineated at 10 min after injection. The gold concentrations in the kidneys, ureter, and bladder at 10 min were 2.59, 5.50, and 5.77 mg/ml, respectively. The number of gold NPs in the kidneys was almost constant between 10 min and 30 min and became too low to determine at 45 min. Presence of gold in the urine and kidneys was confirmed with inductively coupled plasma-mass spectrometry of the organs of a rat euthanized at 25 min after injection. The uptake in the lung, liver, spleen, and heart was lower than that in the kidneys and could be attributed to the presence of blood in these organs because the gold content was almost the same as that in the heart.

MRI in the rats and mice yielded results identical to those obtained with SRCT. Although the Gd(III) content in the Au@DTDTPA-Gd_50_ was lower than the gold content (5 mM versus 50.7 mM), the contrast induced by these particles was higher with MRI than with SRCT. At 45 min after injection, the contrast in the kidneys was still obvious.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Alric C., Taleb J., Le Duc G., Mandon C., Billotey C., Le Meur-Herland A., Brochard T., Vocanson F., Janier M., Perriat P., Roux S., Tillement O. (2008). Gadolinium chelate coated gold nanoparticles as contrast agents for both X-ray computed tomography and magnetic resonance imaging. J Am Chem Soc.
2 Boss A., Bisdas S., Kolb A., Hofmann M., Ernemann U., Claussen C.D., Pfannenberg C., Pichler B.J., Reimold M., Stegger L. (2010). Hybrid PET/MRI of intracranial masses: initial experiences and comparison to PET/CT. J Nucl Med.
3 Cherry S.R. (2006). Multimodality in vivo imaging systems: twice the power or double the trouble?. Annu Rev Biomed Eng.
4 Cherry S.R. (2009). Multimodality imaging: beyond PET/CT and SPECT/CT. Semin Nucl Med.
5 Jennings L.E., Long N.J. (2009). 'Two is better than one'--probes for dual-modality molecular imaging. Chem Commun (Camb).
6 Lee S., Chen X. (2009). Dual-modality probes for in vivo molecular imaging. Mol Imaging.
7 Louie A. (2010). Multimodality imaging probes: design and challenges. Chem Rev.
8 Sanchez P., Valero E., Galvez N., Dominguez-Vera J.M., Marinone M., Poletti G., Corti M., Lascialfari A. (2009). MRI relaxation properties of water-soluble apoferritin-encapsulated gadolinium oxide-hydroxide nanoparticles. Dalton Trans.
9 Park J.A., Kim H.K., Kim J.H., Jeong S.W., Jung J.C., Lee G.H., Lee J., Chang Y., Kim T.J. (2010). Gold nanoparticles functionalized by gadolinium-DTPA conjugate of cysteine as a multimodal bioimaging agent. Bioorg Med Chem Lett.